# Gadolinium-diethylenetriamine tetraacetic acid-icosahedral closo-borane_12_ scaffold

Chemical name: | Gadolinium-diethylenetriamine tetraacetic acid-icosahedral closo-borane_12_ scaffold
Abbreviated name: | CA-9
Synonym: | Gd-DTTA-closo-B_12_ scaffold
Agent category: | Peptide
Target: | Nontargeted
Target category: | Nontargeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally (1). Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field. Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images (2).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (3, 4). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, these low molecular weight MRI contrast agents exhibit low r_1_ relaxivity value (~4 mM^–1^s^–1^ per Gd), high toxicity (nephrogenic systemic fibrosis in patients with renal dysfunction), and a lack of tissue specificity (5). Li et al. (6) have developed polyhedral boranes as a scaffold for the targeted high payload delivery of drugs and imaging agents. A functionalizable monodisperse molecular borane scaffold, [closoB_12_(OH)_12_]^2–^, conjugated with twelve radial ethylene glycol (PEG)_3_ arms with attachments of Gd-labeled diethylenetriamine tetraacetic acid (Gd-DTTA) (CA-9). Goswami et al. (7) evaluated CA-9 for use as a high-performance MRI contrast agent in nude mice bearing human PC-3 prostate tumors.

### Related Resource Links:

- Chapters in MICAD (Gd (http://www.ncbi.nlm.nih.gov/books/?term=Gadolinium+AND+micad%5Bbook%5D))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold+synthesis)]

The 12-fold azidoacetate closomer 7 reacted with the alkyne terminated DTTA-(PEG)_3_ ligand 4 to form DTTA-conjugated closomer 8 with 76% yield (7). Closomer 8 was isolated with column chromatography and then treated with trifluoroacetic acid to remove the tert-butyl ester protecting groups. The deprotected closomer 8 was incubated with GdCl_3_ in a citrate buffer (pH 7) to produce closomer CA-9 with 82% yield. CA-9 was purified with dialysis in ultrapure water. There were 11.3 Gd^3+^ ions per CA-9 as measured with inductively coupled plasma optical emission spectroscopy.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold+in+vitro)]

The average particle size of CA-9 was 12 nm as measured with dynamic laser scattering (7). CA-9 exhibited an r_1_ value (7 T) of 13.8 ± 0.5 mM^–1^s^–1^ per Gd to provide a molar relaxivity value of 155.9 mM^–1^s^–1^. Gd-DTPA-BMA had a molar relaxivity value of 4.2 mM^–1^s^–1^. CA-9 remained >98% intact in bovine serum for 4 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold+rodentia)]

Goswami et al. (7) performed dynamic T1-weighted MRI (7 T) studies with intravenous injection of 0.04 mmol Gd/kg CA-9 or Gd-DTPA-BMA in nude mice (n = 3) bearing PC-3 xenografts. Contrast-enhanced MRI signal intensity (SI) levels were obtained before injection and at 30 min and 60 min after injection. Enhanced contrast in the tumor tissues was visualized for CA-9 at 30 min and 60 min after injection. Contrast enhancement ratios (CERs) [CER = (SI_post_ – SI_pre_)/SI_pre_ X 100%] for CA-9 were 36% and 23% at 30 min and 60 min after injection, respectively. The CERs of tumors for Gd-DTPA-BMA were 19% and 5% at 30 min and 60 min, respectively. Both agents showed high CERs in the kidneys at 30 min, with 70% for CA-9 and 40% for Gd-DTPA-BMA; at 60 min the CERs decreased to 40% and 5%, respectively. Little contrast enhancement was observed for either agent in the liver and muscle at the two time points.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=polyhedral%20borane%20scaffold+human)]

No publication is currently available.

## NIH Support

R21 CA114090

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Burtea, C., S. Laurent, L. Vander Elst, and R.N. Muller, Contrast agents: magnetic resonance. Handb Exp Pharmacol, 2008(185 Pt 1): p. 135-65.
3 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
4 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
5 Laurent S., Elst L.V., Muller R.N. (2006). Comparative study of the physicochemical properties of six clinical low molecular weight gadolinium contrast agents. Contrast Media Mol Imaging.
6 Li T., Jalisatgi S.S., Bayer M.J., Maderna A., Khan S.I., Hawthorne M.F. (2005). Organic syntheses on an icosahedral borane surface: closomer structures with twelvefold functionality. J Am Chem Soc.
7 Goswami L.N., Ma L., Chakravarty S., Cai Q., Jalisatgi S.S., Hawthorne M.F. (2013). Discrete nanomolecular polyhedral borane scaffold supporting multiple gadolinium(III) complexes as a high performance MRI contrast agent. Inorg Chem.